# Cy5-labeled aza-peptidyl Pro-Asn epoxide

Chemical name: | Cy5-labeled aza-peptidyl Pro-Asn epoxide
Abbreviated name: | LP-1
Synonym: | Legumain probe 1
Agent Category: | Compounds
Target: | Legumain/Asparaginyl endopeptidase
Target Category: | Enzyme
Method of detection: | Optical imaging
Source of signal / contrast: | Cy5
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=cysteine+cathepsins)]

Legumain or asparaginyl endopeptidase is a lysosomal cysteine protease that cleaves protein substrates on the C-terminal side of asparagine and, occasionally, aspartic acid residues (1-3). Like other proteases, legumain is synthesized as an inactive zymogen and is activated under acidic conditions in an autocatalytic process (4, 5). Legumain is expressed in diverse cell types and plays a key role in MHC class II–mediated antigen presentation, matrix degradation, and cysteine cathepsin processing (6, 7). Legumain has also been shown to be implicated in various pathological conditions including parasite infection, atherosclerosis, and tumorigenesis (1, 8-10). In mouse models of cancer, knockdown of legumain expression results in a marked decrease in tumor growth and metastasis, while overexpression of legumain leads to increased tumor migration, invasion, and metastasis (1, 11). In human tumors such as carcinomas of the breast, colon, and prostate, legumain has been shown to be overexpressed, while in normal organs like the kidney, liver, and spleen, only a limited quantity of legumain is detectable (10, 11).

Activity-based probes (ABPs) provide a highly versatile means to monitor in vivo protease function and regulation. ABPs utilize irreversible inhibitors that can covalently modify the active site of a protease in an activity-dependent fashion (3, 12, 13). To date, most ABPs have been designed to target cysteine cathepsins and caspases, and only a few legumain-specific probes have been reported in the literature. A typical legumain-specific probe consists of a peptide scaffold, a reactive functional group, and a reporter (1, 14-18). The Cbz-Ala-Ala-Asn peptide is commonly applied as a scaffold, which is designed on the basis of the sequence of a known substrate of legumain. Reactive functional groups, such as aza-Asn halomethylketones, aza-Asn epoxides, and aza-Asn Michael acceptors, have been used to make irreversible legumain binding. In vitro studies have shown that these probes have a high potency against legumain, but they also cross-react with cathepsins and caspases. The in vivo potency and specificity of these probes are largely unknown.

Investigators at Stanford University developed a class of aza-Asn epoxide ABPs with fast kinetic properties and increased selectivity for legumain for use in in vivo imaging studies (1, 3, 16, 19). Some of the probes were also tagged with a series of cell-permeabilizing carriers. These legumain-specific probes showed a high potential for use in imaging active legumain both in normal tissues and solid tumors. In this chapter, legumain probe-1 (LP-1), a Cy5-labeled aza-Pro-Asn epoxide probe, is introduced (1).

### Related Resource Links:

1) Gene information of legumain (http://www.ncbi.nlm.nih.gov/gene/?term=legumain)

2) Legumain-related resource in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=legumain)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Blum+G)]

For comparative analysis, a group of probes have been synthesized and described in detail in several reports (1, 3, 7, 16, 19). These probes included LP-1, LP-1 ctrl, legumain probe-0 (LP-0), legumain inhibitor-1 (LI-1), legumain inhibitor-0 (LI-0), tLP-1, r8 LP-1, penetratin LP-1, and cholesterol LP-1. LP-1 ctrl was the control version of LP-1, which lacks the reactive epoxide group and does not covalently bind to legumain. LP-0 was the Cy5-labeled version of the probe Biotin-PD-AOMK which was developed previously in the same laboratory (18). LI-1 and LI-0 were the acetyl-capped versions of LP-1 and LP-0, respectively. Therefore, LP-1 and LI-1 were aza-epoxide inhibitors, whereas LP-0 and LI-0 were acyloxymethyl ketone (AOMK) inhibitors. The probes of tLP-1, r8 LP-1, penetratin LP-1, and cholesterol LP-1, were the enhanced versions of LP-1, which were generated by conjugating LP-1 with cell-penetrating carriers of tat peptides, cell-penetrating peptides (octa-arginine (r8) and penetratin), and cholesterol, respectively (1). All final products were >97% pure and characterized by either high-resolution mass spectrometry or matrix-assisted laser desorption ionization time-of-flight mass spectrometry. The amounts of impurities were estimated to be minimal (3-7%) (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Blum+G)]

Lee and Bogyo evaluated the potency and selectivity of LI-1 (as a representative of aza-epoxide inhibitors) and LI-0 (as a representative of AOMK inhibitors) against recombinant legumain, cathepsins B and L, and caspase-3 (1). Inhibition studies on the half-maximal inhibitory concentration (IC_50_) showed that LI-1 (IC_50_ = 11.5 nmol) was 70-fold more potent than LI-0 (IC_50_ = 704 nmol) against legumain, whereas both exhibited very weak activity against cathepsin B (IC_50_ = 390 μmol for LI-1 and >1 mmol for LI-0) and cathepsin L (IC_50_ = 220 μmol for LI-1 and >1 mmol for LI-0). LI-0 demonstrated a significant inhibitory effect (IC_50_ = 2.8 μmol) on caspase-3, whereas LI-1 showed nearly no inhibition (IC_50_ = 890 μmol). LI-1 inhibited legumain ~50-fold faster than LI-0 did. These results suggested that incorporation of P1 Asn via an aza-peptidyl scaffold greatly enhanced the efficiency and specificity of aza-epoxide scaffolds compared with that of the P1 Asp AOMK scaffolds. The rapid inhibition kinetics of the aza-Asn epoxide scaffolds may be advantageous for in vivo imaging.

Lee and Bogyo then verified the labeling of active legumain with LP-1 and LP-0 probes in intact NIH-3T3 and RAW 264.7 cells (1). After incubation of the cells with LP-1 and LP-0, SDS-PAGE gel analysis of the cell extracts showed that both probes selectively labeled the active legumain in NIH-3T3 fibroblasts. LP-1 labeled active legumain more efficiently than LP-0, showing an overall stronger labeling signal. However, both probes had some degree of cross-reactivity toward lysosomal cathepsins in RAW 264.7 macrophages. These data suggested that even though probes may have very low potency toward a particular protease target in vitro, when added to cells that actively accumulate the probes in their lysosomes, such as macrophages, they are able to react with other abundant proteases. Furthermore, when RAW 264.7 cells were pretreated with legumain inhibitors, more intense cathepsin labeling was observed. The investigators explained this finding by the fact that cathepsins are substrates of legumain and legumain inhibition could result in increased levels of cathepsins and, therefore, increased nonspecific labeling by the legumain probes.

On the basis of these results, LP-1 was selected for in vivo imaging studies because it has faster kinetics and overall higher potency, resulting in less background labeling of cathepsins and caspases.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

The feasibility of LP-1 for in vivo imaging of active legumain has been tested with the C2C12/Hras1 tumor xenograft model (1). After injection of the LP-1 via tail vein of mice (n = 3), LP-1 rapidly accumulated in tumor tissues, whereas the control probe LP-1 ctrl did not show such accumulation (n = 2 mice). The control probe LP-1 ctrl lacks the reactive epoxide group and therefore does not covalently bind to legumain. The maximum signal/background ratio for LP-1 was reached at ~90 min after injection. The specific legumain signal declined over time but remained significantly higher than the signal observed for LP-1 ctrl, even at the later time points. These data suggested that LP-1 has fast binding and clearance properties. Ex vivo imaging of the tumors and SDS-PAGE analysis of the tumor extracts at the end of the imaging time course confirmed the in vivo selective labeling of legumain by LP-1. The levels of active legumain by imaging directly correlated with the intensity of legumain labeling by SDS-PAGE analysis, which suggests that LP-1 is selective toward legumain in vivo and has virtually no off-target labeling.

Lee and Bogyo further comparatively analyzed LP-1 and the corresponding versions with cell-penetrating carriers (1). In cultured cells, all the carrier-conjugates showed increased cellular uptake and resulted in stronger labeling, but also showed more cross-reactivity with other proteases compared with LP-1. In animal models, enhanced cellular delivery of the conjugates adversely affected their overall circulation, and caused increased association with tissues other than the target tumors, resulting in less useful imaging reagents. These results indicated that legumain ABPs are more effective as free probes that do not contain a carrier peptide.

Lee and Bogyo concluded that they developed a highly potent and selective probe, LP-1, toward active legumain. The favorable reactivity and clearance of LP-1 could result in a high contrast in tumors soon after probe injection. This probe can be used for noninvasive imaging studies of active legumain in whole tissues or cells (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Lee J., Bogyo M. (2010). Development of near-infrared fluorophore (NIRF)-labeled activity-based probes for in vivo imaging of legumain. ACS Chem Biol.
2 Berdowska I. (2004). Cysteine proteases as disease markers. Clin Chim Acta.
3 Bogyo, M., A. Baruch, D.A. Jeffery, D. Greenbaum, A. Borodovsky, H. Ovaa, and B. Kessler, Applications for chemical probes of proteolytic activity. Curr Protoc Protein Sci, 2004Chapter 21: p. Unit 21 17.
4 Mikolajczyk J., Boatright K.M., Stennicke H.R., Nazif T., Potempa J., Bogyo M., Salvesen G.S. (2003). Sequential autolytic processing activates the zymogen of Arg-gingipain. J Biol Chem.
5 Ishizaki, T., A. Erickson, E. Kuric, M. Shamloo, I. Hara-Nishimura, A.R. Inacio, T. Wieloch, and K. Ruscher, The asparaginyl endopeptidase legumain after experimental stroke. J Cereb Blood Flow Metab, 2010
6 Colbert J.D., Matthews S.P., Miller G., Watts C. (2009). Diverse regulatory roles for lysosomal proteases in the immune response. Eur J Immunol.
7 Fonovic M., Bogyo M. (2007). Activity based probes for proteases: applications to biomarker discovery, molecular imaging and drug screening. Curr Pharm Des.
8 Affara N.I., Andreu P., Coussens L.M. (2009). Delineating protease functions during cancer development. Methods Mol Biol.
9 Blum G. (2008). Use of fluorescent imaging to investigate pathological protease activity. Curr Opin Drug Discov Devel.
10 Gawenda J., Traub F., Luck H.J., Kreipe H., von Wasielewski R. (2007). Legumain expression as a prognostic factor in breast cancer patients. Breast Cancer Res Treat.
11 Luo Y., Zhou H., Krueger J., Kaplan C., Lee S.H., Dolman C., Markowitz D., Wu W., Liu C., Reisfeld R.A., Xiang R. (2006). Targeting tumor-associated macrophages as a novel strategy against breast cancer. J Clin Invest.
12 Blum G., von Degenfeld G., Merchant M.J., Blau H.M., Bogyo M. (2007). Noninvasive optical imaging of cysteine protease activity using fluorescently quenched activity-based probes. Nat Chem Biol.
13 Hang H.C., Loureiro J., Spooner E., van der Velden A.W., Kim Y.M., Pollington A.M., Maehr R., Starnbach M.N., Ploegh H.L. (2006). Mechanism-based probe for the analysis of cathepsin cysteine proteases in living cells. ACS Chem Biol.
14 Asgian J.L., James K.E., Li Z.Z., Carter W., Barrett A.J., Mikolajczyk J., Salvesen G.S., Powers J.C. (2002). Aza-peptide epoxides: a new class of inhibitors selective for clan CD cysteine proteases. J Med Chem.
15 James K.E., Gotz M.G., Caffrey C.R., Hansell E., Carter W., Barrett A.J., McKerrow J.H., Powers J.C. (2003). Aza-peptide epoxides: potent and selective inhibitors of Schistosoma mansoni and pig kidney legumains (asparaginyl endopeptidases). Biol Chem.
16 Kato D., Boatright K.M., Berger A.B., Nazif T., Blum G., Ryan C., Chehade K.A., Salvesen G.S., Bogyo M. (2005). Activity-based probes that target diverse cysteine protease families. Nat Chem Biol.
17 Sexton K.B., Kato D., Berger A.B., Fonovic M., Verhelst S.H., Bogyo M. (2007). Specificity of aza-peptide electrophile activity-based probes of caspases. Cell Death Differ.
18 Sexton K.B., Witte M.D., Blum G., Bogyo M. (2007). Design of cell-permeable, fluorescent activity-based probes for the lysosomal cysteine protease asparaginyl endopeptidase (AEP)/legumain. Bioorg Med Chem Lett.
19 Kato D., Verhelst S.H., Sexton K.B., Bogyo M. (2005). A general solid phase method for the preparation of diverse azapeptide probes directed against cysteine proteases. Org Lett.